# CtPyPyIm-(R)^H^_2_^N^γ-PyImPyPy-C_3_-^18^F

Chemical name: | CtPyPyIm-(R)^H^_2_^N^γ-PyImPyPy-C_3_-^18^F
Abbreviated name: | [^18^F]PIPAM8
Synonym:
Agent category: | macromolecule
Target: | DNA
Target category: | Nucleic acid binding molecule
Method of detection: | Positron emission tomography (PET)
Source of signal/contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | No structure is current available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=8-ring hairpin polyamides +18F)]

Polyamides (PAM) constructed from N-methylpyrrole (Py), N-methylimidazole (Im), 3-chlorothiophene (Ct), and N-methylhydroxypyrrole (Hp) amino acids comprise a class of synthetic oligomeric ligands that bind to the minor groove of DNA (1, 2). The aromatic heterocycles in the PAM orientate antiparallel with respect to the Watson-Crick base pair (bp), which leads to a specific recognition of DNA sequences (3). The recognition process follows a series of pairing rules; i.e., an ImPy specifies for G·C, a PyPy binds both A·T and T·A, an HpPy discriminates T·A over A·T, and a CtPy prefers T·A over A·T at the N-terminus. These aromatic amino acids can be programmed to a strand with more than two residues to recognize longer DNA sequences; for example, an ImPyPy motif specifies for the five-bp sequence 5’-WGWCW-3’ (W=A, T) instead of 5’-WGWWW-3’ (4). More complicated PAM motifs can be designed by adding small molecules such as β-alanine or γ-aminobutyric acid to covalently link between two antiparallel PAM strands, yielding substantial increases in affinities and specificities. For instance, an eight-ring hairpin motif, which has a γ-aminobutyric acid (γ-turn) linker to connect the carboxylic terminus of one polyamide to the amino terminus of another, exhibits ~100-fold higher affinity for binding a six-bp DNA sequence compared to the unlinked homodimers (4). PAM motifs are molecules that can permeate cell membranes and have been used in targeting a variety of DNA sequences in cell culture (5). The binding of PAM replaces the DNA-binding proteins and thus regulates the transcription of selected genes. The use of radiolabeled PAM aims at imaging gene regulations in vivo.

Fluorine-18 [^18^F], with a half-life of 109.7 min and low β^+^-energy (0.64 MeV), represents the ideal radionuclide for position emission tomography (PET). The ^18^F-produced positron is annihilated with an electron, leading to the emission of two 511-keV photons ~180º apart, which is detected coincidentally with PET. Various peptides have been successively fluorinated with multistep ^18^F-acylation, using ^18^F-labeled prosthetic groups such as amino-reactive ^18^F-labeling agent N-succinimidyl 4-[^18^F]fluorobenzoate (6). To increase labeling efficiency, the fluorination also can be conducted via a two-step synthetic approach in which an oxime is formed between an aminooxy group in the peptide and an ^18^F-labeled aldehyde such as 4-[^18^F]fluorobenzaldehyde (6). CtPyPyIm-(R)^H^_2_^N^γ-PyImPyPy-C_3_-^18^F ([^18^F]PIPAM8) is an ^18^F-labeled PAM used for PET that is obtained with the oxime ligation approach (5). [^18^F]PIPAM8 contains eight aromatic amino acids connected with a (R)-2,4-diaminobutyric acid, which is denoted as (R)^H^_2_^N^ and is also known as an eight-ring hairpin motif. The use of chiral diaminobutyric acid as the γ-turn increases the overall binding affinity by 10-fold without reduction of sequence specificity (1). PIPAM8 is designed to bind specifically to the sequence 5’-ATACGT-3’ found in the vascular endothelial growth factor (VEGF) hypoxia response element (HRE) and can downregulate the hypoxia-induced VEGF expression in cell culture (7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(8-ring hairpin polyamides +18F)+AND+synthesis%0D%0A)]

Harki et al. reported the synthesis of [^18^F]PIPAM8 (5). Initially, 4-[^18^F]-fluorobenzaldehyde was obtained by nucleophilic fluorination of a trimethylammonium benzaldehyde derivative with cyclotron-produced [^18^F]fluoride in the presence of 5,6-benzo-4,7,13,16,21,24-hexaoxa-1,10-diazabicyclo[8.8.8]hexacos-5-ene (Kryptofix[2.2.2]). The hairpin PAM CtPyPyIm-(R)^H^_2_^N^γ-PyImPyPy was synthesized on a Kaiser oxime resin according to standard protocols. Briefly, after a single Py amino acid and a trimer PyImPy were sequentially loaded on the resin, a chiral turn was introduced via coupling of α-Boc-N-γ-Fmoc-D-diamionbutyric acid, followed by a coupling with a tetramer CtPyPyIm. Then the PAM was hydroxylamine-functionalized in DMF by reaction with tert-butyl-3-aminopropoxycarbamate in the presence of benzotriazolyloxy-tris-(pyrrolidino)-phosphonium hexafluorophosphate (PyBOP) and N,N,-diisopropylethylamine (DIEA). Finally, the obtained CtPyPyIm-(R)^H^_2_^N^γ-PyImPyPy-hydroxylamine was ligated with the 4-[^18^F]-fluorobenzaldehyde with aniline as a catalyst to produce [^18^F]PIPAM8 at radiochemical yield of 7%. The whole synthetic procedure was completed in 100 min after the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(8-ring hairpin polyamides +18F)+AND+%22in+vitro%22)]

Harki et al. used the cold PAM analog [^19^F]PIPAM8 to evaluate its affinity to DNA in vitro (5). Quantitative DNaseI footprint titrations were performed on the 5’-^32^P-polymerase chain reaction fragment from plasmid pGL2-VEGF-Luc. In this method, equilibrium mixtures of ^32^P end-labeled DNA and a range of PAM concentrations were partially digested by DNase I followed by gel electrophoresis and autoradiography. The PAM bound DNA was protected from cleavage, which produced a band gap on the gel. Quantification of the binding fraction as a function of PAM concentration was used to the apparent association constant, 3.3 ± 0.3 × 10^9^ M^-1^ for [^19^F]PIPAM8.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(8-ring hairpin polyamides +18F) +AND++rodentia)]

Harki et al. examined the biodistribution of [^18^F]PIPAM8 in vivo with PET and computed tomography (5). C57 mice were injected intravenously with [^18^F]PIPAM8 at doses of 543, 191, and 84 μCi (20.1, 7.06 and 3.108 MBq), respectively, and PET images were collected for 2 to 3 h. At 4 min after injection, ~36% of injected [^18^F]PIPAM8 was found in the liver and maintained a constant level throughout the duration of PET scan. The excretion from liver to gallbladder was slow; ~5% of injected [^18^F]PIPAM8 was observed in the gastrointestinal tract 20 min after injection. No significant radioactivity was found in the brain, heart, or bone. Thus, the clearance of [^18^F]PIPAM8 was primarily via the liver by excretion through the gallbladder and entry into small intestine; the renal clearance was <1.5%.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(8-ring hairpin polyamides +18F) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(8-ring hairpin polyamides +18F) +AND+human)]

No publication is currently available.

### NIH Support

GM 27681, EB 01943, CA 92865

## References

1 Hsu C.F., Phillips J.W., Trauger J.W., Farkas M.E., Belitsky J.M., Heckel A., Olenyuk B.Z., Puckett J.W., Wang C.C., Dervan P.B. (2007). Completion of a Programmable DNA-Binding Small Molecule Library. Tetrahedron.
2 Nickols N.G., Jacobs C.S., Farkas M.E., Dervan P.B. (2007). Improved nuclear localization of DNA-binding polyamides. Nucleic Acids Res.
3 Belitsky J.M., Nguyen D.H., Wurtz N.R., Dervan P.B. (2002). Solid-phase synthesis of DNA binding polyamides on oxime resin. Bioorg Med Chem.
4 Dervan P.B., Edelson B.S. (2003). Recognition of the DNA minor groove by pyrrole-imidazole polyamides. Curr Opin Struct Biol.
5 Harki D.A., Satyamurthy N., Stout D.B., Phelps M.E., Dervan P.B. (2008). In vivo imaging of pyrrole-imidazole polyamides with positron emission tomography. Proc Natl Acad Sci U S A.
6 Poethko T., Schottelius M., Thumshirn G., Hersel U., Herz M., Henriksen G., Kessler H., Schwaiger M., Wester H.J. (2004). Two-step methodology for high-yield routine radiohalogenation of peptides: (18)F-labeled RGD and octreotide analogs. J Nucl Med.
7 Nickols N.G., Jacobs C.S., Farkas M.E., Dervan P.B. (2007). Modulating hypoxia-inducible transcription by disrupting the HIF-1-DNA interface. ACS Chem Biol.